# [^18^F]3-Fluoro-5-[(2-methyl-1,3-thiazol-4-yl)ethynyl]benzonitrile

Chemical name: | [^18^F]3-Fluoro-5-[(2-methyl-1,3-thiazol-4-yl)ethynyl]benzonitrile
Abbreviated name: | [^18^F]F-MTEB
Synonym:
Agent Category: | Compound
Target: | Metabotropic glutamate subtype 5 (mGlu5) receptor
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=metabotropic%20glutamate%20receptor%20subtype%205%20%28mGluR5%29%20PET%20radiotracers)]

[^18^F]3-Fluoro-5-[(2-methyl-1,3-thiazol-4-yl)ethynyl]benzonitrile ([^18^F]F-MTEB) is a radioligand developed for positron emission tomography (PET) imaging of metabotropic glutamate receptor subtype 5 (mGlu5) in the central nervous system (CNS) (1).

Glutamate is a major excitatory neurotransmitter at CNS synapses. Many neuroanatomical CNS projection pathways contain glutamatergic neurons (2). Glutamate produces its excitatory effects by acting on cell-surface ionotropic glutamate or metabotropic glutamate (mGlu) receptors (3). The mGlu receptors are G-protein-coupled receptors, and the eight mGlu receptor subtypes are further subdivided into groups I, II, and III. The group I receptors include mGlu1 and mGlu5, and they are found mostly in postsynaptic locations. The mGlu5 receptors are found with high to moderate density in the frontal cortex, caudate, putamen, nucleus accumbens, olfactory tubercle, hippocampus, and dorsal horn of the spinal cord, whereas the density in the cerebellum is low. These receptors are coupled to phospholipase C and up- or down-regulate neuronal excitability. They have been implicated in a variety of diseases in the CNS, including anxiety, depression, schizophrenia, Parkinson’s disease, and drug addiction or withdrawal. These receptors are also involved in the modulation of various pain states. They thus are attractive targets for therapeutic drug development.

PET and single-photon emission tomography of radioligands targeting mGlu5 receptors can visualize and study the CNS mGlu5 receptors in normal and pathologic states. Some mGlu5 antagonists have been successfully labeled, but their in vivo visualization has been hampered by high lipophilicity, unfavorable brain uptake kinetics, or a high metabolism (4, 5). 2-Methyl-6-(phenylethynyl)-pyridine (MPEP) and 3-[(2-methyl-1,3-thiazol-4-yl)ethynyl)pyridine (MTEP) have been identified as potent and highly selective noncompetitive antagonists for mGlu5 receptors. Using the structure of MTEP as a template, Hamill et al. (1) and Patel et al (5). designed several MTEP analogs as PET radiotracers, and [^18^F]F-MTEB was one of the compounds that showed high affinity for mGlu5 receptors with moderate lipophilicity.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=metabotropic%20glutamate%20receptor%20subtype%205%20%28mGluR5%29%20PET%20radiotracers%20AND%20synthesis)]

Hamill et al. (1) reported the radiosynthesis of [^18^F]F-MTEB, from the aryl chloride via a nucleophilic aromatic substitution reaction. The precursor was obtained commercially. In the preparation, Kryptofix222 was added to the aqueous [^18^F]F− solution in a microwave cavity. The fluoride was dried under argon gas flow by use of microwave pulses (~45 W). The precursor, in dimethyl sulfoxide, was added to the microwave vial. The reaction mixture was then pulsed with the microwave 5 times at 15 s/pulse and a 30-s pause between pulses. After cooling for 1 min, the reaction was diluted with water and then purified by high-performance liquid chromatography. This procedure gave 259 MBq(7 mC) of [^18^F]F-MTEB with a specific activity (n = 2) of 49.9 ± 17.4 TBq (1,348 ± 469 Ci)/mmol, and a radiochemical purity >98%. The time of synthesis was ~ 35 min with a radiochemical yield of ~4 ± 0.9% (n = 10) at the end of synthesis (uncorrected).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5Bmetabotropic%20glutamate%20receptor%20subtype%205%20%28mGluR5%29%20PET%20radiotracers%20%5D%20AND%20in%20vitro)]

Patel et al. (5) used in vitro rat brain preparations to determine the in vitro mGlu5 binding parameters of unlabeled F-MTEB. [^3^H]MethoxyPyEP, a mGlu5 antagonist, was used in the equilibrium competition studies. The B_max_ for the rat frontal cortex was reported to be 64.7 fmol/mg of tissue (6). The K_i_ of F-MTEB determined from rat cortical membranes was 0.08 ± 0.02 (n = 3) nM, and the partition coefficient (log P) was 3.2 (octanol/buffer, pH 7.4). Hamill et al. (1) reported that the inhibitory concentration (IC_50_; human mGlu5 Ca^2+^ flux assay) was 1.45 ± 0.5 nM (n = 5).

Using a rapid in vitro binding assay they had developed, Patel et al. (7) determined the in vitro regional distribution of [^18^F]F-MTEB in rat and rhesus monkey brain sections. Rat and rhesus brain sections were incubated with [^18^F]F-MTEB and assayed for 20 min, using a no-wash protocol. The percentages of specific binding (n ≥ 2) at 20 min were 69 ± 6.5 and 65 ± 11 for rat and rhesus caudate sections, respectively.

In vitro autoradiographic studies (1) of [^18^F]F-MTEB were carried out in rhesus monkey brain slices (from a single monkey). Good specific to nonspecific regioselective labeling with reasonable binding was found in the cortex, caudate, putamen, amygdale, hippocampus, and most thalamic nuclei. The cerebellar layers showed lower receptor density. In a saturation binding experiment, the B_max_ values for mGlu5 were determined to be 63 and 24 nM in the rhesus caudate and cerebellum, respectively. In vitro metabolism of [^18^F]F-MTEB was studied by incubation of the radiotracer with human and monkey liver microsomes. Liquid chromatography-tandem mass spectrometry showed that the radiotracer was metabolized slowly by human microsomes. Approximately 60% of the intact compound remained at the end of 30 min. In contrast, the compound was metabolized much faster by monkey liver microsomes: only 2% of the intact compound remained at the end of 30 min.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5Bmetabotropic%20glutamate%20receptor%20subtype%205%20%28mGluR5%29%20PET%20radiotracers%20%5D%20AND%20rodents)]

Patel et al. (5) assessed the in vivo distribution of [^18^F]F-MTEB via micro-PET imaging in the rat brain. The rat received ~18.5 MBq (0.5 mCi) of [^18^F]F-MTEB (specific activity ≈ 74 TBq (2,000 Ci)/mmol) by intravenous injection. [^18^F]F-MTEB exhibited the highest uptake (mean normalized activity unit (NAU) of corpus striatum (CS) = 0.64) than other ligands (CS NAUs = 0.19 -0.47) evaluated in the same study and an excellent in vivo specific signal-to-noise ratio. The specific binding and signal-to-noise ratio were reasonably well maintained over 90 min. The corpus striatum/cerebellum ratio was 7. [^18^F]F-MTEB radioactivity specific binding was blocked by a dose of 10 mg/kg MPEP. The blocking dose reduced [^18^F]F-MTEB radioactivity localization in the caudate and cortex to the same level of cerebellum. The dose-inhibition curve estimated the ID_50_ dose of MPEP to be ~1 mg/kg.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5Bmetabotropic%20glutamate%20receptor%20subtype%205%20%28mGluR5%29%20PET%20radiotracers%20%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5Bmetabotropic%20glutamate%20receptor%20subtype%205%20%28mGluR5%29%20PET%20radiotracers%20%5D%20AND%20%28primate%20NOT%20human%29)]

PET imaging with [^18^F]F-MTEB was carried out in three rhesus monkeys (1). Each monkey received ~185 MBq (5 mCi) of the radiotracer. PET showed rapid brain uptake of [^18^F]F-MTEB radioactivity and substantial mGlu5-specific signals in all gray matter regions, including the cerebellum. The wash-out from the brain was relatively slow and thus produced large, long-lived specific signals. The nonspecific signal was determined from the radioactivity in the white matter with a blocking dose of 1 mg/kg MTEP. The total/nonspecific signal ratio at 90 min was 8.4. Coregistered magnetic resonance imaging/PET imaging confirmed that the radioactivity uptake was in the striatum, cortical regions, and cerebellum. The highest concentration of radioactivity was observed in the striatum with ~3.1 standard uptake value (SUV) units at ~65 min. Radioactivity uptake was lower in the frontal cortex and even lower in the cerebellum. These uptakes were blocked by MTEP pretreatment. The distribution of radioactivity seen in PET imaging was consistent with the in vitro autoradiography pattern.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5Bmetabotropic%20glutamate%20receptor%20subtype%205%20%28mGluR5%29%20PET%20radiotracers%20%5D%20AND%20human)]

No publication is currently available.

## References

1 Hamill TG, Krause S, Ryan C, Bonnefous C, Govek S, Seiders TJ, Cosford ND, Roppe J, Kamenecka T, Patel S, Gibson RE, Sanabria S, Riffel K, Eng W, King C, Yang X, Green MD, O'Malley SS, Hargreaves R, Burns HD. (2005). Synthesis, characterization, and first successful monkey imaging studies of metabotropic glutamate receptor subtype 5 (mGluR5) PET radiotracers. Synapse.
2 Pin JP, Duvoisin R. (1995). The metabotropic glutamate receptors: structure and functions. Neuropharmacology.
3 Slassi A, Isaac M, Edwards L, Minidis A, Wensbo D, Mattsson J, Nilsson K, Raboisson P, McLeod D, Stormann TM, Hammerland LG, Johnson E. (2005). Recent advances in non-competitive mGlu5 receptor antagonists and their potential therapeutic applications. Curr Top Med Chem.
4 Ametamey SM, Kessler LJ, Honer M, Wyss MT, Buck A, Hintermann S, Auberson YP, Gasparini F, Schubiger PA. (2006). Radiosynthesis and Preclinical Evaluation of 11C-ABP688 as a Probe for Imaging the Metabotropic Glutamate Receptor Subtype 5. J Nucl Med.
5 Patel S, Ndubizu O, Hamill T, Chaudhary A, Burns HD, Hargreaves R, Gibson RE. (2005). Screening cascade and development of potential Positron Emission Tomography radiotracers for mGluR5: in vitro and in vivo characterization. Mol Imaging Biol.
6 Patel S, Krause SM, Hamill T, Chaudhary A, Burns DH, Gibson RA. (2003). In vitro characterization of [3H]MethoxyPyEP, an mGluR5 selective radioligand. Life Sci.
7 Patel S, Hamill T, Hostetler E, Burns HD, Gibson RE. (2003). An in vitro assay for predicting successful imaging radiotracers. Mol Imaging Biol.